# [carbonyl-^11^C](R,S)-(N-(2-(1-(4-(2-Methoxyphenyl)piperazinyl)(2-methylethyl)))-N-pyridinyl)cyclohexanecarboxamide

Chemical name: | [carbonyl-^11^C](R,S)-(N-(2-(1-(4-(2-Methoxyphenyl)piperazinyl)(2-methylethyl)))-N-pyridinyl)cyclohexane-carboxamide
Abbreviated name: | [carbonyl-^11^C](R,S)-JWAY
Synonym: | [^11^C]JWAY, {^11^C](R,S)-JWAY
Agent Category: | Compound
Target: | 5-HT_1A_ receptors
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=JWAY%20OR%20%5Bcarbonyl-11C%5D%28R%2CS%29-JWAY)]

[carbonyl-^11^C](R,S)-(N-(2-(1-(4-(2-Methoxyphenyl)piperazinyl)(2-methylethyl)))-N-pyridinyl)cyclohexanecarboxamide ([carbonyl-^11^C](R,S)-JWAY) is a radioligand developed for positron emission tomography (PET) imaging of serotonin-1A (5-HT_1A_) receptors in the central nervous system (1). It is a selective 5-HT_1A_ antagonist labeled with ^11^C, a positron emitter with a physical t_½_ of 20.4 min (2).

The serotonin (5-hydroxytryptamine (5-HT)) neurotransmission system comprises mainly neurons in the brainstem, with nerve tracts extending from these neurons to many areas of the brain and spinal cord (3). When neurons fire, they release 5-HT, a neurotransmitter that is involved in the modulation of various important physiologic functions and behavior, such as thermoregulation, cardiovascular function, aggressive and sexual behavior, mood, appetite, and the sleep–wake cycle (4). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which also contain several subtypes (5). There are five receptor subtypes within the G protein-coupled 5-HT_1_ receptor family, with the 5-HT_1A_ subtype located primarily in the limbic forebrain (the hippocampus, entorhinal cortex ,septum, and raphe) (4, 5). 5-HT_1A_ receptors appear to function both as presynaptic (somatodendritic) autoreceptors in the raphe nuclei and as postsynaptic receptors in the terminal fields. This receptor subtype is involved in the modulation of emotion and the function of the hypothalamus, and is implicated in the pathogenesis of anxiety, depression, hallucinogenic behavior, motion sickness, dementia, schizophrenia, and eating disorders (6). A radioligand that can be used to assess the in vivo densities of 5-HT_1A_ receptors and their changes may facilitate investigation of the relationship of these receptors to various neuropsychiatric diseases and aid in the design of novel drugs for their treatment.

Many psychiatric drugs modulate serotonergic transmission or specifically target the 5-HT_1A_ receptors (2). Various compounds have been radiolabeled for visualization and quantification of these receptors (7). WAY 100635 was developed as a highly selective, silent antagonist (possessing no intrinsic agonist activity) of 5HT_1A_ receptors at both pre- and postsynaptic sites. WAY 100635 radiolabeled with ^11^C at the carbonyl position is an effective radioligand but it is rapidly cleared and metabolized. Analogs of WAY100635 bearing bulkier cycloalkylcarbonyl groups appear to be more resistant to amide hydrolysis. However, the added lipophilicity also reduces receptor affinity (8). McCarron et al. (1) proposed adding a smaller group to WAY-100635 for less impact on lipophilicity and receptor affinity. They synthesized (R,S)-JWAY by adding a methyl group (α-carbon position to the carbonyl group) on the ethyl side chain of WAY100635. This WAY-100635 analog was radiolabeled with ^11^C and evaluated with PET in a monkey. The radioligand gave a high 5-HT_1A_ receptor-selective PET signal, but the added methyl group did not appear to have the desired influence on the rate of metabolism.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28JWAY%20OR%20%5B11C-carbonyl%5D%28R%2CS%29JWAY%29%20AND%20synthesis)]

.McCarron et al. (1) reported the synthesis of (R,S)-JWAY from commercially available 2-methoxyphenyl piperazine in four steps. 2-Methoxyphenyl piperazine was first reacted with α-chloro-propionyl chloride in anhydrous tetrahydrofuran (THF) and triethylamine at room temperature overnight to give 1-(2-chloro-propionyl)-4-(2-methoxyphenyl)piperazine with a yield of 83%. In the second step, this amide was added to 2-aminopyridine in potassium-t-butoxide and anhydrous N,N-dimethylformamide at room temperature overnight to produce an intermediate compound with a yield of 89%. In the third step, this compound was reacted with lithium aluminum hydride in diethyl ether at room temperature overnight to produce 1-(2-methoxyphenyl)-4-((2-methyl)-2-(2-aminopyridinyl)ethyl)piperazine with a yield of 79%. The final step involved reacting this compound with cyclohexanecarbonyl chloride in THF at room temperature overnight. (R,S)-JWAY was produced from this final step with a yield of 60%. This compound was used as a precursor for the radiosynthesis of [carbonyl-^11^C](R,S)-JWAY.

The radiosynthesis method involved acylation of the precursor with [^11^C]cyclohexanecarbonyl chloride (1). The procedure used immobilized cyclohexylmagnesium chloride as a Grignard reagent in a long polypropylene tube to trap ^11^CO_2_ and to obtain the desired [carbonyl-^11^C]cyclohexanecarbonyl chloride (by passing thionyl chloride through the tube) (9). The radioligand was separated by high-performance liquid chromatography (HPLC) with 98% decay-corrected radiochemical yields. Radiochemical purity of [carbonyl-^11^C](R,S)-JWAY was >99%. The specific activity at the time of injection was 6.99 GBq/μmol (189 Ci/mmol) in the baseline experiments and 8.51 GBq/μmol (230 Ci/mmol) in the pretreatment experiments.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28JWAY%20OR%20%5B11C-carbonyl%5D%28R%2CS%29JWAY%29%20AND%20in%20vitro)]

McCarron et al. (1) computed the n-octanol-water partition (logP) and distribution coefficients for all charged and neutral species between octanol and buffer at pH 7.4 (log D) values of (R,S)-JWAY from drawn molecular structures using a software program. These values were 3.81 and 3.08 for logP and LogD, respectively. In comparison, the calculated values for WAY-100635 were 3.28 and 2.88, respectively. The binding affinity (K_i_) value of (R,S)-JWAY was 0.91 nM based on the inhibition of binding of [^3^H]5-carboxamidotryptamine to cloned human 5-HT_1A_ receptors in vitro. WAY-100635 had a K_i_ value of 0.37 nM.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28JWAY%20OR%20%5B11C-carbonyl%5D%28R%2CS%29JWAY%29%20AND%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28JWAY%20OR%20%5B11C-carbonyl%5D%28R%2CS%29JWAY%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28JWAY%20OR%20%5B11C-carbonyl%5D%28R%2CS%29JWAY%20%29%20AND%20%28primate%20NOT%20human%29)]

[carbonyl-^11^C](R,S)-JWAY was evaluated by PET imaging in a male cynomolgus monkey (1). The animal received 54 MBq (1.46 mCi) of (carbonyl-^11^C](R,S)-JWAY (7.72 nmol, 3.36 μg) by i.v. administration. In the baseline study, in which only the radioligand was injected, radioactivity uptake in the whole brain reached a maximum of 4.8% of the injected dose at 2.5 min and decreased to 1.2% at 90 min. Clearance was more rapid from the cerebellum than from 5-HT_1A_ receptor−rich regions. At 90 min, the ratios of 5-HT_1A_ receptor−rich regions to cerebellum were 2.60 (cingulated cortex), 2.58 (hippocampus), 2.20 (frontal cortex), and 2.15 (temporal cortex), and these ratios were still increasing. When the animal was pretreated with WAY-100635 (0.5 mg/kg), the retention of [carbonyl-^11^C](R,S)-JWAY radioactivity in 5-HT_1A_ receptor−rich regions was reduced to the same level as in the receptor-devoid cerebellum. The 90-min ratios were reduced to 1.42 (cingulated cortex), 1.27 (hippocampus), 1.22 (frontal cortex), and 1.07 (temporal cortex).

In the metabolite analysis, (carbonyl-^11^C](R,S)-JWAY radioactivity cleared rapidly from the monkey blood with a t_½_ of 7.8 min, and the radioligand appeared to be rapidly metabolized (1). In both the baseline and pretreatment studies, about 64% and 12% of (carbonyl-^11^C](R,S)-JWAY remained in the plasma at 4 min and 45 min, respectively. The HPLC analysis of the plasma showed two radioactive metabolites were present, and both of them were more polar than (carbonyl-^11^C](R,S)-JWAY. This was consistent with amide hydrolysis of (carbonyl-^11^C](R,S)-JWAY as the primary route of metabolism. In comparison, (carbonyl-^11^C]WAY-100635 was reported to have 69% and 19% of the injected dose in monkey plasma at the same time points (1, 10).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28JWAY%20OR%20%5B11C-carbonyl%5D%28R%2CS%29JWAY%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIH intramural support.

## References

1 McCarron J.A., Marchais-Oberwinkler S., Pike V.W., Tarkiainen J., Halldin C., Sovago J., Gulyas B., Wikstrom H.V., Farde L. (2005). Two C-methyl derivatives of [11C]WAY-100635--effects of an amido alpha-methyl group on metabolism and brain 5-HT1A receptor radioligand behavior in monkey. Mol Imaging Biol.
2 Bantick R.A., Rabiner E.A., Hirani E., de Vries M.H., Hume S.P., Grasby P.M. (2004). Occupancy of agonist drugs at the 5-HT1A receptor. Neuropsychopharmacology.
3. Sunderland, P.M., Structure and function of the nervous system, in Pathophysiology: The biologic basis for disease in adults and children, K.L. McCance, and S.H. Huether, Editor. 1994, Mosby-Year Book, Inc.: St. Louis, MO. p. 397-436.
4 Passchier J., van Waarde A. (2001). Visualisation of serotonin-1A (5-HT1A) receptors in the central nervous system. Eur J Nucl Med.
5 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
6 Lang L., Jagoda E., Schmall B., Vuong B.K., Adams H.R., Nelson D.L., Carson R.E., Eckelman W.C. (1999). Development of fluorine-18-labeled 5-HT1A antagonists. J Med Chem.
7 Tauscher J., Verhoeff N.P., Christensen B.K., Hussey D., Meyer J.H., Kecojevic A., Javanmard M., Kasper S., Kapur S. (2001). Serotonin 5-HT1A receptor binding potential declines with age as measured by [11C]WAY-100635 and PET. Neuropsychopharmacology.
8 Houle S., DaSilva J.N., Wilson A.A. (2000). Imaging the 5-HT(1A) receptors with PET: WAY-100635 and analogues. Nucl Med Biol.
9 McCarron J., Turton D.R., Pike V.W., Poole K.G. (1996). Remotely controlled production of the 5-HT1A receptor radioligand, [carbonyl-11C]WAY100635, via 11C-carboxylation of an immobilized Grignard reagent. J. Labelled Compd. Radiopharm.
10 Osman S., Lundkvist C., Pike V.W., Halldin C., McCarron J.A., Swahn C.G., Farde L., Ginovart N., Luthra S.K., Gunn R.N., Bench C.J., Sargent P.A., Grasby P.M. (1998). Characterisation of the appearance of radioactive metabolites in monkey and human plasma from the 5-HT1A receptor radioligand, [carbonyl-11C]WAY-100635--explanation of high signal contrast in PET and an aid to biomathematical modelling. Nucl Med Biol.